# ^111^In-1,4,7-Triazacyclononane,1-glutaric acid-4,7-acetic acid-Glu-[cyclo(Arg-Gly-Asp-D-Phe-Lys)]_2_

Chemical name: | ^111^In-1,4,7-Triazacyclononane,1-glutaric acid-4,7-acetic acid-Glu-[cyclo(Arg-Gly-Asp-D-Phe-Lys)]_2_
Abbreviated name: | ^111^In-NODAGA-E-[c(RGDfK)]_2_
Synonym:
Agent category: | Peptide
Target: | Integrin α_v_β_3_
Target category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT), gamma planar imaging
Source of signal: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=23831237), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=56237028) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=ShowDetailView&TermToSearch=3678&ordinalpos=5&itool=EntrezSystem2.PEntrez.Gene.Gene_ResultsPanel.Gene_RVDocSum) for more information about integrin α_v_.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NODAGA%20c(RGDfK))]

Integrins are a family of heterodimeric glycoproteins on cell surfaces that mediate diverse biological events involving cell–cell and cell–matrix interactions (1). Integrins consist of an α and a β subunit and are important for cell adhesion and signal transduction. The α_v_β_3_ integrin is the most prominent receptor affecting tumor growth, tumor invasiveness, metastasis, tumor-induced angiogenesis, inflammation, osteoporosis, and rheumatoid arthritis (2-7). Expression of the α_v_β_3_ integrin is strong on tumor cells and activated endothelial cells, whereas expression is weak on resting endothelial cells and most normal tissues. Antagonists of α_v_β_3_ are being studied as antitumor and antiangiogenic agents, and the agonists of α_v_β_3_ are being studied as angiogenic agents for coronary angiogenesis (6, 8, 9). Extracellular matrix proteins (vitronectin, fibrinogen, laminin, and collagen) contain a tripeptide sequence consisting of Arg-Gly-Asp (RGD), which binds to a variety of integrins, including α_v_β_3_. Various radiolabeled antagonists have been introduced for use with the imaging of tumors and tumor angiogenesis (10).

Most cyclic RGD peptides are composed of five amino acids. Haubner et al. (11) reported that various cyclic RGD (c(RGD)) peptides exhibit selective inhibition of binding to α_v_β_3_ (inhibition concentration (IC_50_), 7–40 nM) but not to integrins α_v_β_5_ (IC_50_, 600–4,000 nM) or α_IIb_β_3_ (IC_50_, 700–5,000 nM). Various radiolabeled c(RGD) peptides have been found to have high accumulation in tumors in nude mice (12). Dijkgraaf et al. (13) reported the evaluation of ^111^In-1,4,7-triazacyclononane,1-glutaric acid-4,7-acetic acid-Glu-[cyclo(Arg-Gly-Asp-D-Phe-Lys)]_2_ (^111^In-NODAGA-E-[c(RGDfK)]_2_) for use with single-photon emission computed tomography (SPECT) imaging of α_v_β_3_ in tumors.

### Related Resource Links:

- Chapters in MICAD (RGD (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=RGD+AND+micad%5Bbook%5D))
- Gene information in NCBI (α_v_ integrin (http://www.ncbi.nlm.nih.gov/gene/3685), β_3_ integrin (http://www.ncbi.nlm.nih.gov/gene/3690))
- Articles in Online Mendelian Inheritance in Man (OMIM) (α_v_ integrin (http://www.ncbi.nlm.nih.gov/omim/193210), β_3_ integrin (http://www.ncbi.nlm.nih.gov/omim/173470))
- Clinical trials (RGD (http://www.clinicaltrials.gov/ct2/results?term=RGD))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NODAGA%20c(RGDfK)+synthesis)]

Dijkgraaf et al. (13) prepared the synthesis of ^111^In-NODAGA-E-[c(RGDfK)]_2_ by reacting NODAGA-E-[c(RGDfK)]_2_ with 1–20 MBq (0.027–0.54 mCi) ^111^InCl_3_ in 2-(N-morpholino)ethanesulfonic acid buffer (pH 5.5) for 15 min at 100°C. Radiochemical purity was >98% as determined with high-performance liquid chromatography, with an overall yield of 91%. The specific activity was 2.2–40 MBq/nmol (0.059–1.08 mCi/nmol) at the end of purification. ^111^In-NODAGA-E-[c(RGDfK)]_2_ had a logP value of −4.34 ± 0.09.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NODAGA%20c(RGDfK)+in+vitro)]

Dijkgraaf et al. (13) performed in vitro solid-phase binding assays of ^111^In-DOTA-E-[c(RGDfK)]_2_ with human α_v_β_3_ integrin. NODAGA-E-[c(RGDfK)]_2_ had an IC_50_ value of 0.043 ± 0.037 nM. DOTA-E-[c(RGDfK)]_2_ had an IC_50_ value of 0.037 ± 0.085 nM.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NODAGA%20c(RGDfK)+rodentia)]

Dijkgraaf et al. (13) performed ex vivo biodistribution studies of 0.4 MBq (11 µCi) ^111^In-NODAGA-E-[c(RGDfK)]_2_ with nude mice (n = 3–5/group) bearing SK-RC-52 human renal carcinoma tumors at 2 h after injection. The tumor accumulation was 5.0 ± 0.6% injected dose/gram (ID/g). The organ with the highest accumulation was the kidney (5.0% ID/g), followed by the intestine (2.5% ID/g), spleen (1.7% ID/g), stomach (1.6%), and liver (1.5% ID/g). Low accumulation (<1% ID/g) was observed in the muscle, heart, lung, stomach, pancreas, and femur. Very low radioactivity was detected in blood (<0.1% ID/g). Coinjection of excess NODAGA-E-[c(RGDfK)]_2_ resulted in 88% reduction of radioactivity in the tumor (P < 0.001). The accumulation was also reduced in the liver, lung, intestine, stomach, femur, and spleen (this may be partly mediated by α_v_β_3_ integrin in these tissues), but the kidney was not affected. SPECT scans showed that the tumor was clearly visualized at 2 h after injection of 10–20 MBq (0.27–0.54 mCi) ^111^In-NODAGA-E-[c(RGDfK)]_2_. Some accumulation was observed in the kidneys. Coinjection of excess NODAGA-E-[c(RGDfK)]_2_ reduced radioactivity in the tumor but not in the kidney.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NODAGA%20c(RGDfK)+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NODAGA%20c(RGDfK)+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NODAGA%20c(RGDfK)+human)]

No publication is currently available.

## References

1 Hynes R.O. (1992). Integrins: versatility, modulation, and signaling in cell adhesion. Cell.
2 Jin H., Varner J. (2004). Integrins: roles in cancer development and as treatment targets. Br J Cancer.
3 Varner J.A., Cheresh D.A. (1996). Tumor angiogenesis and the role of vascular cell integrin alphavbeta3. Important Adv Oncol.
4 Wilder R.L. (2002). Integrin alpha V beta 3 as a target for treatment of rheumatoid arthritis and related rheumatic diseases. Ann Rheum Dis.
5 Grzesik W.J. (1997). Integrins and bone--cell adhesion and beyond. Arch Immunol Ther Exp (Warsz).
6 Kumar C.C. (2003). Integrin alpha v beta 3 as a therapeutic target for blocking tumor-induced angiogenesis. Curr Drug Targets.
7 Ruegg C., Dormond O., Foletti A. (2002). Suppression of tumor angiogenesis through the inhibition of integrin function and signaling in endothelial cells: which side to target?. Endothelium.
8 Kerr J.S., Mousa S.A., Slee A.M. (2001). Alpha(v)beta(3) integrin in angiogenesis and restenosis. Drug News Perspect.
9 Mousa S.A. (2003). alphav Vitronectin receptors in vascular-mediated disorders. Med Res Rev.
10 Haubner R., Wester H.J. (2004). Radiolabeled tracers for imaging of tumor angiogenesis and evaluation of anti-angiogenic therapies. Curr Pharm Des.
11 Haubner R., Wester H.J., Burkhart F., Senekowitsch-Schmidtke R., Weber W., Goodman S.L., Kessler H., Schwaiger M. (2001). Glycosylated RGD-containing peptides: tracer for tumor targeting and angiogenesis imaging with improved biokinetics. J Nucl Med.
12 Chen X., Park R., Shahinian A.H., Tohme M., Khankaldyyan V., Bozorgzadeh M.H., Bading J.R., Moats R., Laug W.E., Conti P.S. (2004). 18F-labeled RGD peptide: initial evaluation for imaging brain tumor angiogenesis. Nucl Med Biol.
13 Dijkgraaf I., Terry S.Y., McBride W.J., Goldenberg D.M., Laverman P., Franssen G.M., Oyen W.J., Boerman O.C. (2013). Imaging integrin alpha-v-beta-3 expression in tumors with an (18) F-labeled dimeric RGD peptide. Contrast Media Mol Imaging.